# [^18^F]Fluorocholine

Chemical name: | [^18^F]Fluorocholine
Abbreviated name: | [^18^F]FCH, FCH
Synonym: | [^18^F]Fluoromethyl-dimethyl-2-hydroxyethylammonium; [^18^F]fluoromethylcholine
Agent category: | Compound
Target: | Choline kinases
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluorocholine)]

Choline is an important component of phospholipids in the cell membranes. Tissues with increased metabolism will lead to an increased uptake of choline. Choline is phosphorylated by choline kinases (CHK) to phosphorylcholine within cells, and, after several biosynthetic processes, finally is integrated into phospholipids (1). Because tumor cells have a high metabolic rate, choline uptake is high in order to keep up with the demands with the synthesis of phospholipids in their cellular membranes (2).

Positron emission tomography (PET) with [^11^C]choline has been reported to be useful for the detection and differential diagnosis of brain tumors, prostate cancer, lung cancer, and esophageal cancer (3). However, [^11^C]choline has a high uptake in liver, kidney, and spleen. [^18^F]-labeled choline analog was initially synthesized as [^18^F]fluoroethylcholine to replace [^11^C]choline as a PET tracer due to the short physical half-life of ^11^C (4). Although ^18^F has a longer half-life (110 min), [^18^F]fluoroethylcholine showed a rapid accumulation in the urinary bladder, rendering it less desirable for imaging prostate cancer and pelvic lymph nodes. Therefore, [^18^F]fluorocholine (FCH) was conceived to be a better biological analog than [^18^F]fluoroethylcholine (5). FCH PET studies showed high uptake in malignancies in patients with prostate cancer, breast carcinoma, and brain tumors (6, 7).

### Related Resource Links:

- Chapters in MICAD (Choline (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=choline+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Choline kinase (http://www.ncbi.nlm.nih.gov/gene/1119))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Choline kinase (http://www.ncbi.nlm.nih.gov/omim/612395))
- Clinical trials (Fluorocholine (http://www.clinicaltrials.gov/ct2/results?term=fluorocholine))
- Drug information in FDA (Fluorocholine (http://google2.fda.gov/search?q=fluorocholine&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluorocholine%20and%20synthesis)]

[^18^F]Choline was synthesized from [^18^F]fluorobromomethane and dimethylethanolamine with a radiochemical purity greater than 98% and a radiochemical yield (not corrected for decay) for the synthesis and purification was approximately 20-40% (5). An automated method of FCH synthesis was achieved by the reaction of [^18^F]fluoromethyl triflate with dimethylethanolamine on a Sep-Pak column. The total time required for obtaining the finished chemical was 30 min. The radiochemical yield (decay corrected) was 80% with the radiochemical purity and chemical purity of > 98% (8).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluorocholine%20AND%20in%20vitro)]

The radiochemical purity of FCH was found to be stable at room temperature for 7 hours and at 37ºC in human whole blood for 2 hours. Both [^14^C]choline and FCH was phosphorylated by yeast CHK. Cultured PC-3 human prostate cells accumulated FCH at a slightly lower rate than FDG. The FCH uptake and phosphorylation were inhibited by a CHK inhibitor, HC-3. Approximate 72% of radioactivity was in phosphocholine and 25% of radioactivity was in lipophilic metabolites after two hours of incubation with PC-3 cells (6).

## Animal Studies

### Rodent Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluorocholine%20AND%20rodentia)]

In a murine PC-3 xenograft model, ex vivo biodistribution of FDG, [^14^C]choline and FCH were compared. FCH showed a similar biodistribution to [^14^C]choline in the tumor-bearing mouse, with prominent uptake in kidney, liver, lung, and heart. No differences were observed in the biodistribution pattern in normal tissues of control and tumor-bearing mice. Tumor uptake of FCH was similar to [^14^C]choline and FDG in the mouse model, however, tumor-to-blood ratios were moderately higher for FCH (9).

### Other Non-Primate Mammal Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluorocholine%20AND%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primate Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluorocholine%20AND%20primate%20NOT%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluorocholine%20AND%20human)]

FCH was cleared from blood in the first 5 min after administration in humans. The radioactivity in the liver increased rapidly in the first 10 min and then gradually thereafter. The FCH PET scan of 12 normal human subjects showed the highest uptake in the kidneys, liver, and spleen. Human dosimetry was estimated based on murine and human biodistribution data. The kidneys received the highest dose of radioactivity, followed by the bladder, liver, and spleen (10). The effective dose equivalent of administration of 4.07 MBq/kg (0.11 mCi/kg) is about 0.03 mSv/MBq (0.1 rad/mCi).

PET imaging studies of cancer patients showed the feasibility of FCH uptake in prostate cancer, breast cancer, and brain tumors. Osseous, soft tissue and lymph node metastases were also detected by FCH uptake foci (5, 6). Two recent prostate cancer studies with a total of 36 patients showed that malignant tumors, recurrent tumors and lymph node metastases could be localized with FCH PET scans (11, 12). However, Schmid et al. (12) noted that differentiation of benign hyperplasia from malignant prostate lesions was not possible with FCH PET.

## References

1 Zeisel S.H., Blusztajn J.K. (1994). Choline and human nutrition. Annu Rev Nutr.
2 Podo F. (1999). Tumour phospholipid metabolism. NMR Biomed.
3 Hara T. (2002). 11C-choline and 2-deoxy-2-[18F]fluoro-D-glucose in tumor imaging with positron emission tomography. Mol Imaging Biol.
4 Hara T., Yuasa M. (1997). Automated synthesis of fluorine-18 labeled choline analogue: 2-fluoroetheyl-dimethyl-2-oxyethylammonium. J Nucl Med.
5 DeGrado T.R., Coleman R.E., Wang S., Baldwin S.W., Orr M.D., Robertson C.N., Polascik T.J., Price D.T. (2001). Synthesis and evaluation of 18F-labeled choline as an oncologic tracer for positron emission tomography: initial findings in prostate cancer. Cancer Res.
6 DeGrado T.R., Baldwin S.W., Wang S., Orr M.D., Liao R.P., Friedman H.S., Reiman R., Price D.T., Coleman R.E. (2001). Synthesis and evaluation of (18)F-labeled choline analogs as oncologic PET tracers. J Nucl Med.
7 Hara T., Kondo T., Hara T., Kosaka N. (2003). Use of 18F-choline and 11C-choline as contrast agents in positron emission tomography imaging-guided stereotactic biopsy sampling of gliomas. J Neurosurg.
8 Iwata R., Pascali C., Bogni A., Furumoto S., Terasaki K., Yanai K. (2002). [18F]fluoromethyl triflate, a novel and reactive [18F]fluoromethylating agent: preparation and application to the on-column preparation of [18F]fluorocholine. Appl Radiat Isot.
9 Price D.T., Coleman R.E., Liao R.P., Robertson C.N., Polascik T.J., DeGrado T.R. (2002). Comparison of [18 F]fluorocholine and [18 F]fluorodeoxyglucose for positron emission tomography of androgen dependent and androgen independent prostate cancer. J Urol.
10 DeGrado T.R., Reiman R.E., Price D.T., Wang S., Coleman R.E. (2002). Pharmacokinetics and radiation dosimetry of 18F-fluorocholine. J Nucl Med.
11 Kwee S.A., Coel M.N., Lim J., Ko J.P. (2005). Prostate cancer localization with 18fluorine fluorocholine positron emission tomography. J Urol.
12 Schmid D.T., John H., Zweifel R., Cservenyak T., Westera G., Goerres G.W., von Schulthess G.K., Hany T.F. (2005). Fluorocholine PET/CT in patients with prostate cancer: initial experience. Radiology.